# ^66^Ga-Labeled PEGylated nano-graphene oxide (GO) covalently linked to NOTA-conjugated anti-CD105 (endoglin) chimeric monoclonal antibody TRC105

Chemical name: | ^66^Ga-Labeled PEGylated nano-graphene oxide (GO) covalently linked to NOTA-conjugated anti-CD105 (endoglin) chimeric monoclonal antibody TRC105
Abbreviated name: | [^66^Ga]-NOTA-GO-TRC105
Synonym:
Agent Category: | Antibody
Target: | CD105 (endoglin) antigen
Target Category: | Antigen
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^66^Ga
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=CD105&cmd=DetailsSearch)]

The CD105 antigen (endoglin) is a hypoxia-inducible, 180-kDa, disulfide-linked, homodimeric transmembrane glycoprotein that is a co-receptor for the transforming growth factor β (TGF-β) (1). Both CD105 and TGF-β are expressed at low levels in resting endothelial cells, but they are overexpressed in cancerous lesions and play a significantly proangiogenic role in remodeling the vasculature of malignant tumors (2). It has been shown that the levels of CD105 in endothelial tissues correlate well with the degree of cell proliferation and that the antigen is a suitable biomarker to quantify tumor angiogenesis and can be used to determine the prognostic outcome for cancer patients (3). The biological activity of CD105 has been discussed in detail by Seon et al. (4). Investigators have demonstrated that immunotoxins and radioimmunoconjugates generated with anti-CD105 monoclonal antibodies (mAbs) can inhibit angiogenesis and prevent the growth and metastasis of cancerous tumors (4). For translation to the clinic, a human/mouse chimeric anti-CD105 mAb (designated c-SNj6 or TRC105) was generated and shown to have suitable pharmacokinetic, toxicological, and immunogenicity characteristics for use in non-human primates (5). Currently, a clinical trial (http://clinicaltrials.gov/ct2/show/NCT01326481?term=endoglin&rank=5) is in progress to evaluate the use of TRC105 for the treatment of metastatic breast cancer.

TRC105 has been labeled with ^64^Cu (6) and ^89^Zr (7), respectively, and has been reported to detect the expression of CD105 with positron emission tomography (PET) imaging in xenograft tumors in mice. In another study, TRC105 was conjugated to IRDye 800CW, a near-infrared fluorescent (NIRF) dye, and the expression of CD105 in tumors was visualized with NIRF imaging (8). TRC105 has also been conjugated with ^64^Cu and IRDye 800CW to develop a dual-modality (PET/NIRF) imaging agent that can be used to detect murine breast cancer 4T1 (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CRL-2539&Template=cellBiology) cell tumors in mice (9). Recently, TRC105 was conjugated to 1,4,7-triazacyclononane-1,4,7-triacetic acid (NOTA) and labeled with ^66^Ga, and the radioimmunoconjugate was shown to be suitable to visualize the expression of CD105 with PET in 4T1 cell tumors in mice (10).

Investigators have recently become interested in the use of PEGylated graphene oxide (GO; to read about the physical and chemical properties of graphene, see Feng and Liu (11)), a carbon-based material, in biomedical applications such as drug delivery (12), cancer therapy (13), and preclinical in vivo imaging and ablation of tumors in mice (14). Hong et al. used PET to evaluate ^66^Ga-labeled PEGylated nano-GO covalently linked to NOTA-conjugated TRC105 ([^66^Ga]-NOTA-GO-TRC105) to visualize and target tumors that express the CD105 antigen in mice (15).

### Related Resource Links

TRC105 (http://www.ncbi.nlm.nih.gov/books/?term=TRC105+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books) chapters in MICAD

Other anti-CD105 antibody chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=Anti-CD105+antibody+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Human CD105 (endoglin) protein and mRNA (http://www.ncbi.nlm.nih.gov/nuccore/BC014271.2) sequences

CD105 gene information (http://www.ncbi.nlm.nih.gov/gene/2022) (Gene ID: 2022)

CD105 in Online Mendelian Inheritance in Man Database (http://omim.org/entry/131195) (OMIM)

Clinical trials (http://www.clinicaltrials.gov/ct2/results?term=TRC105) related to TRC105

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B66Ga%5D-NOTA-GO-TRC105%20synthesis&cmd=DetailsSearch)]

The ^66^Ga used to perform the work described in this chapter was produced by the bombardment of either ^nat^Zn or ^66^Zn as described by Hong et al. (15). When ^nat^Zn was used to produce ^66^Ga, the final preparation of the nuclide contained <5% ^67^Ga (t_1/2_ = 78.3 h) as a contaminant. The purity of ^66^Ga produced from ^66^Zn was reported to be >99.9%.

NOTA-GO and NOTA-GO-TRC105 were produced for radiolabeling with ^66^Ga and utilized in the PET imaging and biodistribution studies as described elsewhere (15). Fluorescein isothiocyanate (FITC)-labeled GO (FITC-GO) and FITC-GO-TRC105 were synthesized to investigate the in vitro CD105 binding affinity and specificity of the complexes with fluorescence techniques (15). The average number of NOTA or TRC105 molecules covalently linked to a sheet of GO was not reported. The average small sheet size range of NOTA-GO and NOTA-GO-TRC105 was 10–50 nm, and this size range was confirmed with dynamic light scattering (DLS) analysis. The average diameters of the two GO conjugates were 21.9 ± 0.6 nm and 27.0 ± 0.9 nm, respectively, as determined with DLS (15). The zeta-potentials of NOTA-GO and NOTA-GO-TRC105 were determined to be −9.46 ± 4.74 mV and 0.08 ± 5.35 mV, respectively.

NOTA-GO and NOTA-GO-TRC105 were respectively labeled with ^66^Ga, and the radiolabeled products were purified with size-exclusion chromatography using phosphate-buffered saline containing 0.25 M ammonium acetate (pH 7.2) as the mobile phase (15). The final radiolabeled preparations were passed through a 0.22-μm filter for use in in vivo studies. The radiochemical yields, radiochemical purities, and specific activities of [^66^Ga]-NOTA-GO and [^66^Ga]-NOTA-GO-TRC105 were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B66Ga%5D-NOTA-GO-TRC105%20in%20vitro&cmd=DetailsSearch)]

The stability of [^66^Ga]-NOTA-GO and [^66^Ga]-NOTA-GO-TRC105 was investigated by incubating the tracers in complete mouse serum at 37°C for up to 24 h, and the incubation mixtures were sampled at various time points to determine the percentage of radioactivity retained on the GO conjugates (15). Both ^66^Ga-labeled GO conjugates were reported to retain >97% radioactivity at all the time points, suggesting that the radiolabeled complexes would have excellent in vivo stability.

Flow cytometric analysis of HUVEC (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CRL-1730&Template=cellBiology) cells (human umbilical vein endothelial cells that have a high expression of CD105) exposed to 50 μg/mL FITC-GO-TRC105 (based on GO content) showed that the cells had >600-fold higher fluorescence intensity compared with the untreated cells (15). Cells blocked with 3.33 nmol TRC105 and then treated with FITC-GO-TRC105 as above had ~100-fold lower fluorescence intensity compared with cells exposed to FITC-GO-TRC105 alone. This indicated that FITC-GO-TRC105 bound specifically to the CD105 antigen on the HUVEC cells. Minimal fluorescence was observed in MCF-7 (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=HTB-22&Template=cellBiology) cells (a human breast cancer epithelial cell line that does not express CD105; used a negative control in this study), indicating that FITC-GO-TRC105 exhibited low non-specific binding to the cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B66Ga%5D-NOTA-GO-TRC105%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^66^Ga]-NOTA-GO and [^66^Ga]-NOTA-GO-TRC105 was investigated in mice bearing murine breast cancer 4T1 (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CRL-2539&Template=cellBiology) cell tumors as described by Hong at al (15). The animals (n = 4 mice/group) were given an injection of the tracer (dose not mentioned) through the tail vein and euthanized at 3 h postinjection (p.i.). All the major organs, including the tumors, were retrieved from the animals to determine the amount of radioactivity accumulated in the various tissues. Data obtained from the study were presented as percent of injected dose per gram tissue (% ID/g). With both radiolabeled GO conjugates, radioactivity was detected mainly in the liver (~10.5% ID/g), followed by the blood (~7.5% ID/g), spleen (~12% ID/g and ~7.5% ID/g with [^66^Ga]-NOTA-GO-TRC105 and [^66^Ga]-NOTA-GO, respectively), and the tumors (~6.5% ID/g and ~3.5% ID/g with [^66^Ga]-NOTA-GO-TRC105 and [^66^Ga]-NOTA-GO, respectively; P < 0.05) at 3 h p.i. All other organs showed a radioactivity uptake of <2.5% ID/g with either tracer. Tumors of mice injected with [^66^Ga]-NOTA-GO-TRC105 showed a significantly higher uptake of label (~4.0% ID/g; P < 0.05) compared with the amount of radioactivity detected in the tumors of mice injected with [^66^Ga]-NOTA-GO (~2.5% ID/g). Another group of mice (n = 4 animals) that were given a blocking dose of NOTA-GO-TRC105 (33.33 nmol/kg body weight) before injecting the radiolabeled GO conjugate showed a significantly lower accumulation of radioactivity in the tumors at 24 h p.i. (~1.5% ID/g) compared with the lesions of animals injected with [^66^Ga]-NOTA-GO-TRC105 alone (~4.5% ID/g; P < 0.05). This indicated that the ^66^Ga-labeled NOTA-GO-TRC105 complex had a high binding specificity for the CD105 antigen (15).

For PET imaging of mice bearing 4T1 cell tumors (n = 4 animals), the rodents were injected with 5–10 MBq (135–270 μCi) [^66^Ga]-NOTA-GO-TRC105 or [^66^Ga]-NOTA-GO through the tail vein, and static whole-body images of the animals were acquired at 0.5 h, 3 h, 7 h, and 24 h p.i (15). Quantitative data were obtained from the images with region-of-interest analysis as described by Hong et al. (15). The amount of tracer in the blood was 10.9 ± 1.4% ID/g, 7.5 ± 1.2% ID/g, 5.3 ± 1.1% ID/g, and 3.4 ± 0.4% ID/g at 0.5, 3, 7, and 24 h p.i., respectively, and the amount of label in the liver was 10.7 ± 1.7% ID/g, 11.4 ± 1.5% ID/g, 10.4 ± 1.3% ID/g, and 8.0 ± 1.1% ID/g at 0.5, 3, 7, and 24 h p.i. respectively. The tumors were clearly visible at 0.5 h p.i. and showed an uptake of 3.8 ± 0.4% ID/g, 4.5 ± 0.4% ID/g, 5.8 ± 0.3% ID/g, and 4.5 ± 0.4% ID/g at 0.5, 3, 7, and 24 h p.i. respectively. The accumulation of radioactivity in the muscles with [^66^Ga]-NOTA-GO-TRC105 was <0.5% ID/g at all the time points. In general, with [^66^Ga]-NOTA-GO the level and pattern of radioactivity uptake in the liver and blood were similar to those with [^66^Ga]-NOTA-GO-TRC105. With [^66^Ga]-NOTA-GO, the level of tracer in the tumors was high at all time points (~3.0% ID/g) but significantly lower (P < 0.05) than that observed with [^66^Ga]-NOTA-GO-TRC105. The investigators attributed the increased accumulation of radioactivity with [^66^Ga]-NOTA-GO in the 4T1 tumors to the enhanced permeability and retention effect in the lesions (15).

To determine the in vivo target-binding specificity of [^66^Ga]-NOTA-GO-TRC105, the animals (n = 4 mice) were injected with 13.3 nmol nonradioactive TRC105 2 h before administration of the ^66^Ga-labeled GO conjugate (15). PET images of the animals were acquired as before. The uptake of label in the tumors was 1.3 ± 0.3% ID/g, 1.5 ± 0.2% ID/g, 1.1 ± 0.3% ID/g, and 1.2 ± 0.1% ID/g at 0.5, 3, 7, and 24 h p.i., respectively, which was significantly lower (P < 0.05 at all the time points) than the accumulation observed in the lesions of animals injected with [^66^Ga]-NOTA-GO-TRC105 alone (for uptake values, see above). Although the amount of radioactivity in the liver of animals given the blocking dose was similar to that of animals injected with [^66^Ga]-NOTA-GO-TRC105 alone at all the time points (9.0 ± 1.8% ID/g, 10.8 ± 2.0% ID/g, 10.0 ± 1.9% ID/g, and 10.2 ± 1.9% ID/g at 0.5, 3, 7, and 24 h p.i. respectively), the level of tracer in the blood of animals pretreated with TRC105 was lower (6.0 ± 1.2% ID/g, 3.4 ± 0.8% ID/g, 2.0 ± 0.3% ID/g, and 2.0 ± 0.3% ID/g at 0.5, 3, 7, and 24 h p.i., respectively). Therefore, this study confirmed the in vivo CD105 binding specificity of the GO-radioimmunoconjugate.

To confirm the uptake of NOTA-GO-TRC105 in CD105-specific tissues of mice bearing 4T1 cell tumors, the animals (n = 3 mice) were injected with 5 mg/kg body weight of the non-radiolabeled GO-immunoconjugate and euthanized at 3 h p.i. to remove the tumors, liver, spleen, and muscles of the rodents (15). The harvested tissues were then frozen and cryo-sectioned for histological examination. High levels of NOTA-GO-TRC105 were observed as dark spots only in tissue sections of the tumors, liver, and spleen, but not in the muscle of these animals. However, NOTA-GO was observed only in the sections of liver and spleen tissues obtained from animals injected with the GO-chelating agent complex. This study demonstrated that NOTA-GO-TRC105 specifically targets the CD105 antigen in the tumor. Immunofluorescence staining of the tissue slices for CD31 (a biomarker for the vasculature), with anti-mouse CD31 as the primary antibody and for CD105 using the TRC105 within NOTA-GO-TRC105 as the primary antibody, showed that the uptake of NOTA-GO-TRC105 in the liver and spleen was due to the non-specific capture of the complex by the reticuloendothelial system and not due to the specific targeting of CD105 on the vasculature. Almost no uptake of NOTA-GO-TRC105 was observed in the muscles and other normal tissues of the animals.

From these studies, the investigators concluded that [^66^Ga]-NOTA-TRC105 is a suitable agent to detect tumors that express the CD105 antigen in rodents (15).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B66Ga%5D-NOTA-GO-TRC105%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B66Ga%5D-NOTA-GO-TRC105%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B66Ga%5D-NOTA-GO-TRC105%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## NIH Support

This work was supported in part by a grant from the National Institutes of Health through the UW Radiological Sciences Training Program 5 T32 CA009206-32.

## References

1 Nassiri F., Cusimano M.D., Scheithauer B.W., Rotondo F., Fazio A., Yousef G.M., Syro L.V., Kovacs K., Lloyd R.V. (2011). Endoglin (CD105): a review of its role in angiogenesis and tumor diagnosis, progression and therapy. Anticancer Res.
2 Perez-Gomez E., Del Castillo G., Juan Francisco S., Lopez-Novoa J.M., Bernabeu C., Quintanilla M. (2010). The role of the TGF-beta coreceptor endoglin in cancer. ScientificWorldJournal.
3 Fonsatti E., Nicolay H.J., Altomonte M., Covre A., Maio M. (2010). Targeting cancer vasculature via endoglin/CD105: a novel antibody-based diagnostic and therapeutic strategy in solid tumours. Cardiovasc Res.
4 Seon B.K., Haba A., Matsuno F., Takahashi N., Tsujie M., She X., Harada N., Uneda S., Tsujie T., Toi H., Tsai H., Haruta Y. (2011). Endoglin-targeted cancer therapy. Curr Drug Deliv.
5 Shiozaki K., Harada N., Greco W.R., Haba A., Uneda S., Tsai H., Seon B.K. (2006). Antiangiogenic chimeric anti-endoglin (CD105) antibody: pharmacokinetics and immunogenicity in nonhuman primates and effects of doxorubicin. Cancer Immunol Immunother.
6 Hong H., Yang Y., Zhang Y., Engle J.W., Barnhart T.E., Nickles R.J., Leigh B.R., Cai W. (2011). Positron emission tomography imaging of CD105 expression during tumor angiogenesis. Eur J Nucl Med Mol Imaging.
7 Hong H., Severin G.W., Yang Y., Engle J.W., Zhang Y., Barnhart T.E., Liu G., Leigh B.R., Nickles R.J., Cai W. (2012). Positron emission tomography imaging of CD105 expression with 89Zr-Df-TRC105. Eur J Nucl Med Mol Imaging.
8 Yang Y., Zhang Y., Hong H., Liu G., Leigh B.R., Cai W. (2011). In vivo near-infrared fluorescence imaging of CD105 expression during tumor angiogenesis. Eur J Nucl Med Mol Imaging.
9 Zhang Y., Hong H., Engle J.W., Yang Y., Theuer C.P., Barnhart T.E., Cai W. (2012). Positron Emission Tomography and Optical Imaging of Tumor CD105 Expression with a Dual-Labeled Monoclonal Antibody. Mol Pharm.
10 Engle J.W., Hong H., Zhang Y., Valdovinos H.F., Myklejord D.V., Barnhart T.E., Theuer C.P., Nickles R.J., Cai W. (2012). Positron emission tomography imaging of tumor angiogenesis with a (66)ga-labeled monoclonal antibody. Mol Pharm.
11 Feng L., Liu Z. (2011). Graphene in biomedicine: opportunities and challenges. Nanomedicine (Lond).
12 Yang K., Wan J., Zhang S., Zhang Y., Lee S.T., Liu Z. (2011). In vivo pharmacokinetics, long-term biodistribution, and toxicology of PEGylated graphene in mice. ACS Nano.
13 Yang K., Zhang S., Zhang G., Sun X., Lee S.T., Liu Z. (2010). Graphene in mice: ultrahigh in vivo tumor uptake and efficient photothermal therapy. Nano Lett.
14 Zhang W., Guo Z., Huang D., Liu Z., Guo X., Zhong H. (2011). Synergistic effect of chemo-photothermal therapy using PEGylated graphene oxide. Biomaterials.
15 Hong H., Zhang Y., Engle J.W., Nayak T.R., Theuer C.P., Nickles R.J., Barnhart T.E., Cai W. (2012). In vivo targeting and positron emission tomography imaging of tumor vasculature with (66)Ga-labeled nano-graphene. Biomaterials.